# Dimethylamino-3(4-[^11^C]methoxyphenyl)-3H-pyrido[3',2':4,5]thieno[3,2-d]pyrimidin-4-one

Chemical name: | Dimethylamino-3(4-[^11^C]methoxyphenyl)-3H-pyrido[3',2':4,5]thieno[3,2-d]pyrimidin-4-one
Abbreviated name: | [^11^C]MMTP, [^11^C]1
Synonym:
Agent category: | Compound
Target: | Metabotropic glutamate receptor subtype 1 (mGluR1)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11C%20MMTP)]

Glutamate is a major excitatory neurotransmitter at neuronal synapses in the central nervous system (CNS) (1, 2). Glutamate produces its excitatory effects by acting on cell-surface ionotropic glutamate or metabotropic glutamate receptors (mGluRs). The mGluRs are GTP-binding protein (G-protein)–coupled receptors that play important roles in regulating the activity of many synapses in the CNS, and many neuronal projection pathways contain mGluRs. There are eight mGluR subtypes, which are further subdivided into groups I, II, and III. The group I receptors include mGluR1 and mGluR5, and they are found predominantly in postsynaptic locations. The mGluR1 is found in moderate to high density in the cerebellum, caudate, putamen, thalamus, cingulate cortex, and hippocampus, with low density in the pons. The mGluR5 is usually found in moderate to high density in the frontal cortex, caudate, putamen, nucleus accumbens, olfactory tubercle, and hippocampus, whereas the density in the cerebellum is low. The mGluR1 and mGluR5 are positively coupled to phospholipase C in the regulation of neuronal excitability (3). Dysfunction of mGluR1 and mGluR5 is implicated in a variety of diseases in the CNS, including anxiety, depression, schizophrenia, Parkinson’s disease, and drug addiction or withdrawal (2, 4).

Positron emission tomography (PET) and single-photon emission tomography of radioligands targeting the mGluR1 can visualize and analyze mGluR1 expression in normal physiological and pathological conditions. Several radioligands have been studied for in vivo imaging of the mGluR1 in the brain (5). Dimethylamino-3(4-methoxyphenyl)-3H-pyrido[3',2':4,5]thieno[3,2-d]pyrimidin-4-one (MMTP) was shown to be selective for the mGluR1, with nanomolar affinity (K_i_ = 7.9 nM), and exhibited little inhibition of the mGluR5. Prabhakaran et al. (6) prepared and evaluated dimethylamino-3(4-[^11^C]methoxyphenyl)-3H-pyrido[3',2':4,5]thieno[3,2-d]pyrimidin-4-one ([^11^C]MMTP) for use with in vivo PET imaging of mGluR1 distribution in the brain of baboons.

### Related Resource Links:

- Chapters in MICAD (mGluR1 (http://www.ncbi.nlm.nih.gov/books?Db=books&Cmd=DetailsSearch&Term=mGluR1+AND+micad%5Bbook%5D), mGluR5 (http://www.ncbi.nlm.nih.gov/books?term=mGluR5%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (mGluR1 (http://www.ncbi.nlm.nih.gov/gene/2911), mGluR5 (http://www.ncbi.nlm.nih.gov/gene/2915))
- Articles in Online Mendelian Inheritance in Man (OMIM) (mGluR1 (http://omim.org/entry/604473), mGluR5 (http://www.ncbi.nlm.nih.gov/omim/604102))
- Clinical trials (mGluR1 (http://www.clinicaltrials.gov/ct2/results?term=mGluR1), mGluR5 (http://www.clinicaltrials.gov/ct2/results?term=mglur5))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20MMTP%20and%20synthesis)]

Prabhakaran et al. (6) synthesized [^11^C]MMTP by O-methylation of the desmethyl precursor dimethylamino-3(4-hydroxyphenyl)-3H-pyrido[3',2':4,5]thieno[3,2-d]pyrimidin-4-one with [^11^C]methyl trifluoromethanesulfonate (MeOTf) at 25°C for 5 min. Subsequent separation with high-performance liquid chromatography produced a radiochemical purity >99%. The radiochemical yield was 30% based on [^11^C]MeOTf, and specific activity was 111–185 GBq/μmol (3–5 Ci/µmol; n = 6) at the end of synthesis. The total synthesis time was not reported. [^11^C]MMTP exhibited a log P value of 3.15.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20MMTP%20and%20in%20vitro)]

In vitro [^11^C]MMTP (12 nM) autoradiographic imaging studies were performed on postmortem human brain sections (n = 4/group) (6). JNJ-16259685 (a selective mGluR1 antagonist, 10 µM) was used to determine non-specific binding. [^11^C]MMTP bound heterogeneously to the brain sections, with the highest accumulation of radioactivity in the mGluR1-rich cerebellum (B_max_ = 140 ± 20 fmol/cm^2^), followed by the hippocampus (B_max_ = 110 ± 25 fmol/cm^2^), frontal cortex (B_max_ = 85 fmol/cm^2^), and striatum (B_max_ = 20 fmol/cm^2^). JNJ-16259685 completely blocked radioactive signals to background levels in these brain regions.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20MMTP%20and%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20MMTP%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20MMTP%20and%20%28primate%20not%20human%29)]

Prabhakaran et al. (6) performed dynamic PET imaging studies for 90 min in baboons (number of animals studied not reported) after intravenous injection of 175 MBq (5 mCi, 2 nmol) [^11^C]MMTP. Baseline tissue time-activity curves revealed a high accumulation of radioactivity in the cerebellum. However, the caudate, amygdala, putamen, hippocampus, and frontal cortex exhibited lower radioactivity levels and faster washout than the cerebellum. The radioactivity levels of these brain regions were similar. The ratios of cerebellum to most of the other brain regions were 2.0, 1.7, and 1.6 at 35, 65, and 85 min after injection, respectively. [^11^C]MMTP remained 45% and 30% intact in the plasma at 30 min and 90 min, respectively. No blocking studies were performed.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20MMTP%20and%20human)]

No publication is currently available.

## NIH Support

R21 MH081801

## References

1 Pin J.P., Duvoisin R. (1995). The metabotropic glutamate receptors: structure and functions. Neuropharmacology.
2 Ferraguti F., Crepaldi L., Nicoletti F. (2008). Metabotropic glutamate 1 receptor: current concepts and perspectives. Pharmacol Rev.
3 Abe T., Sugihara H., Nawa H., Shigemoto R., Mizuno N., Nakanishi S. (1992). Molecular characterization of a novel metabotropic glutamate receptor mGluR5 coupled to inositol phosphate/Ca2+ signal transduction. J Biol Chem.
4 Gasparini F., Lingenhohl K., Stoehr N., Flor P.J., Heinrich M., Vranesic I., Biollaz M., Allgeier H., Heckendorn R., Urwyler S., Varney M.A., Johnson E.C., Hess S.D., Rao S.P., Sacaan A.I., Santori E.M., Velicelebi G., Kuhn R. (1999). 2-Methyl-6-(phenylethynyl)-pyridine (MPEP), a potent, selective and systemically active mGlu5 receptor antagonist. Neuropharmacology.
5 Yamasaki T., Fujinaga M., Yoshida Y., Kumata K., Yui J., Kawamura K., Hatori A., Fukumura T., Zhang M.R. (2011). Radiosynthesis and preliminary evaluation of 4-[18F]fluoro-N-[4-[6-(isopropylamino)pyrimidin-4-yl]-1,3-thiazol-2-yl]-N-methylb enzamide as a new positron emission tomography ligand for metabotropic glutamate receptor subtype 1. Bioorg Med Chem Lett.
6 Prabhakaran J., Majo V.J., Milak M.S., Kassir S.A., Palner M., Savenkova L., Mali P., Arango V., Mann J.J., Parsey R.V., Kumar J.S. (2010). Synthesis, in vitro and in vivo evaluation of [11C]MMTP: a potential PET ligand for mGluR1 receptors. Bioorg Med Chem Lett.